# 4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-pyridinyl)-p-[^18^F]fluorobenzamido]ethylpiperazine

Chemical name: | 4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-pyridinyl)-p-[^18^F]fluorobenzamido]ethylpiperazine
Abbreviated name: | p-[^18^F]MPPF
Synonym: | [^18^F]FBWAY, [^18^F]MPPF
Agent Category: | Compound
Target: | 5-HT_1A_ receptors
Target Category: | Receptor-ligand binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal /contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18%20MPPF)]

4-(2´-Methoxyphenyl)-1-[2´-(N-2´´-pyridinyl)-p-[^18^F]fluorobenzamido]ethylpiperazine (p-[^18^F]MPPF) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-HT_1A_) receptors in the central nervous system (1). It is a selective 5-HT_1A_ radiotracer labeled with ^18^F, a positron emitter with a physical t_½_ of 110 min (2).

The serotonin (5-hydroxytryptamine (5-HT)) neurotransmission system consists mainly of neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord (3). During firing, the neurons release 5-HT, a neurotransmitter that is involved in the modulation of various important physiologic functions and behavior, such as thermoregulation, cardiovascular function, aggressive and sexual behavior, mood, appetite, and the sleep–wake cycle. The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which also contain several subtypes. There are five receptor subtypes within the G protein–coupled 5-HT_1_ receptor family, and the 5-HT_1A_ subtype is located primarily in the limbic forebrain (the hippocampus, entorhinal cortex, and septum). 5-HT_1A_ appears to function both as a presynaptic (somatodendritic) autoreceptor in the raphe nuclei and as a postsynaptic receptor in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors. Many compounds have been radiolabeled and studied for visualization and quantification of these receptors by PET or single-photon emission computed tomography (SPECT). WAY 100635 has been developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5HT_1A_ receptors at both pre- and postsynaptic sites. Zhuang et al. (4, 5) first developed a series of arylpiperazine-benzamido derivatives and 4-(2´-methoxyphenyl)-1-[2´-[N-(2´´-pyridinyl)-p-iodobenzamido]ethyl]piperazine ([^125^I]MPPI), which appeared to selectively bind to the 5-HT_1A_ receptors in vitro and in vivo. Their studies showed that various benzoyl substituents affected the inhibition constant (K_i_) of the compound. Zhuang et al. (4) also synthesized a fluoro analog, p-MPPF, that displayed a high binding affinity for 5-HT_1A_ receptors and acted as a receptor antagonist in vivo. In 1994, Shiue et al. (6) synthesized p-[^18^F]MPPF for PET studies of 5-HT_1A_ receptors in humans.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20synthesis)]

Zhuang et al. (5) synthesized p-MPPI as well as the fluoro analog of p-MPPF. The procedure involved the initial condensation of 2-aminopyridine with chloroacetyl chloride and then acylation with 2-chloro-N-(2-pyridyl)-acetamide. The subsequent reduction to the amine as the key intermediate compound gave an 81% overall yield. Coupling of the acyl groups with this intermediate compound was accomplished with an acyl chloride in the presence of triethylamine or by the use of acids with oxalyl chloride in dimethyl formamide. Both reactions gave yields of 50-90%. Using this approach, Shiue et al. (6) synthesized p-[^18^F]MPPF by first preparing the nitro compound of 4-(2´-methoxyphenyl)-1-[2´-(N-2”-pyridinyl)-p-nitrobenzamido]ethylpiperazine (p-MPPNO_2_), and then used nucleophilic substitution of the nitro group with [^18^F]fluoride. [^18^F]Fluoride was prepared by the ^18^O(p,n)^18^F reaction on an enriched water target added to a solution of K_2_CO_3_/Kryptofix 2.2.2. The nitro compound in dimethyl sulfoxide was added to the dried K[^18^F], and the mixture was kept at 140°C for 20 min. The final compound was purified by use of a C_18_ Sep-Pak column and then by high-performance liquid chromatography (HPLC). The synthesis time was 90 min, and the radiochemical yield was 10% at 90 min from the end of bombardment (EOB). Specific activity was 37-148 GBq (1-4 Ci)/µmol at the end of synthesis (EOS).

Le Bars et al. (7) used microwave heating at 3 min/500 W and a remotely controlled process for the radiosynthesis. They also reported better separation between the fluorinated compound and its nitro precursor with the use of a ternary solvent mixture of tetrahydrofuran, methanol, and aqueous sodium acetate for the HPLC. The synthesis time was shortened to 70 min, and the radiochemical yield was 25% at EOS. The specific activity averaged about 37-185 GBq (1-5 Ci)/µmol at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20in%20vitro)]

Zhuang et al. (4, 5) reported a K_i_ for p-[^18^F]MPPF of 3.2 ± 0.8 nM with use of rat hippocampal homogenates and ^125^I-labeled trans-8-hydroxy-2-(N-n-propyl-N-3´-iodo-2´-propenyl)aminotetralin ([^125^I]-(R)-(+)-trans-8-OH-PIPAT). In comparison, WAY 100635 had a K_i_ of 0.84 ± 0.1 nM. Kung et al. (8) synthesized [^3^H] p-[^18^F]MPPF by a [^3^H]CH_3_I methylation reaction for binding studies in rat hippocampal membrane homogenates. The K_d_ was 0.34 ± 0.12 nM, and the B_max_ was 145 ± 35 fmol/mg protein. Autoradiographic studies of rat brain sections showed that [^3^H] p-[^18^F]MPPF localization was similar to the distribution of 5-HT_1A_ receptors. Ma et al. (9) studied the metabolites of p-[^18^F]MPPF and other fluorinated WAY analogs with use of rat hepatocytes and human liver tissue. They identified the major metabolites by liquid chromatography–tandem mass spectrometry and found significant between-species differences in metabolism. In rat hepatocytes, the aromatic ring oxidation was the major metabolism pathway. For human hepatocytes, amide hydrolysis products were the major metabolites. They also reported significant differences among different fluorinated analogs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20rodentia)]

Shiue et al. (6) studied the tissue distribution of p-[^18^F]MPPF in rats, using a dose of 925-1110 kBq (25-30 µCi). The brain radioactivity was 0.7% injected dose (ID)/g at 2 min and then decreased rapidly. The washout rates of radioactivity were slower in regions (e.g., hippocampus, cerebral cortex, and hypothalamus) with high concentrations of 5-HT_1A_ receptors than in regions that lacked these receptors. The maximum hippocampus/cerebellum ratio was 5.6 at 30 min. Treatment with (±)8-hydroxy-2-di-n-propylamino-tetralin ((±)-8-OH-DPAT), a 5-HT_1A_ agonist (2 mg/kg i.v.), or WAY 100635 (a 5-HT_1A_ antagonist; 1 mg/kg i.v.) 5 min before radiotracer administration significantly reduced the radioactivity in the serotonergic regions. In a rat biodistribution study, Lang et al. (10) reported DUR [(%ID/g) × body weight (g)/100] values (n ≥ 4) for p-[^18^F]MPPF of 0.165 ± 0.023, 0.377 ± 0.100, and 0.066 ± 0.008 in the cortex, hippocampus, and cerebellum, respectively. The hippocampus/cerebellum DUR ratio was 4.7 and decreased to 2.1 with a 50-nmol injection of WAY 100635.

In two in vivo tests of hypothermia and reciprocal forepaw treading in rats, Thielen et al. (11) confirmed that p-MPPF acts as a 5-HT_1A_ receptor antagonist. In a similar study (11), the same research group found that p-MPPF behaved as a competitive antagonist of both postsynaptic 5-HT_1A_ receptors and somatodendritic 5-HT_1A_ autoreceptors. Lang et al. (12) studied the metabolite profile of p-[^18^F]MPPF in rat brain and blood, and they reported that the radioactivity (3700 kBq (100 µCi)) was extracted with high efficiency (84-92%). In the brain distribution, radioactivity had an early rapid net efflux from the whole brain and appeared to have two components (10). The t_½_ (second component) of the whole brain was 35 min. The metabolite-corrected blood t_½_ was 41 min. In a blocking experiment involving injection of 50 nmol of WAY 100536, p-[^18^F]MPPF showed only ~60% reduction of specific binding in the hippocampus.

Plenevaux et al. (13) studied the in vivo behavior of p-[^18^F]MPPF in awake, freely moving rats, using a radioactivity dose of 37-185 MBq ((1-5 mCi); specific activity = 55.5 ±18.5 GBq/µmol (1.5 ± 0.5 Ci/µmol) at the EOS). After injection, plasma clearance was fast, and the plasma clearance rate was constant (k = -0.028 ± 0.007 min^-1^) between 15 and 60 min. The highest concentrations of radioactivity were found in the liver and kidney. In the brain, the total radioactivity was cleared at a constant rate (k = -0.044 ± 0.010 min^-1^) from 0.113 ± 0.019% ID at 15 min to 0.018 ± 0.002% ID at 60 min. At 30 min, the radioactivities in the hippocampus and frontal cortex were 1.7 and 4 times (n = 12) higher than in the cerebellum and striatum, respectively. Between 15 and 60 min, 70-90% of the radioactivity was p-[^18^F]MPPF, as determined by HPLC analyses of the brain tissue. In the plasma, as much as 60% of the total radioactivity at 60 min came from metabolites. Qualitative comparisons between ex vivop-[^18^F]MPPF and in vitro [^3^H]-OH-DPAT autoradiographic labeling showed that the same rat brain regions were labeled.

Passchier et al. (14) showed that p-[^18^F]MPPF was a substrate for P-glycoprotein in experiments using wild-type and mdr1a(–/–) knockout mice. Using a positron-sensitive intracerebral probe and microdialysis in rats, Zimmer et al. (15, 16) found that p-[^18^F]MPPF binding could be modulated by modifications of extracellular serotonin in the rat hippocampus. The same group of researchers showed that p-[^18^F]MPPF specific binding was significantly enhanced after a decrease in extracellular serotonin and that the binding was also sensitive to electrically evoked serotonin release (17, 18).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Le Bars et al. (7) injected 55.5 MBq (1.5 mCi) of p-[^18^F]MPPF into adult female cats. PET imaging revealed high levels of radioactivity in the limbic cortex (including the hippocampus) and cingulate cortex. Time-activity curves showed high initial radioactivity localization in all brain regions, followed by a rapid washout. The washout rates were lower in the cingulated and limbic cortices than in the cerebellum. Pretreatment with WAY 100635 (500 µg/kg) 30 min before radiotracer injection completely blocked localization of p-[^18^F]MPPF radioactivity in the serotonergic regions.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5D-MPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20%28primate%20NOT%20human%29)]

Shiue et al. (6) performed PET brain imaging with p-[^18^F]MPPF in a male cynomologus monkey. An i.v. bolus dose of 150 MBq (4.06 mCi) was given, and PET scans showed localization and retention of radioactivity in the monkey’s hippocampus. The ratio of radioactivity in the hippocampus to that in the cerebellum was 3 at 30 min after injection. This ratio was reduced to 1 by the injection of (±)-8-OH-DPAT (2 mg/kg i.v.) 23 min after injection of p-[^18^F]MPPF in the displacement experiment. Plasma metabolite analyses showed that the appearance of metabolites in the plasma was relatively rapid. Only 23% of radioactivity in the monkey plasma remained as p-[^18^F]MPPF at 30 min after injection. Carson et al. (19) performed brain imaging of [^18^F]fluorobenzoic acid, a major metabolite of p-[^18^F]MPPF, in rhesus monkeys. [^18^F]Fluorobenzoic acid was taken up by the monkey brain, but HPLC analysis of arterial blood showed no metabolites for [^18^F]fluorobenzoic acid.

Udo De Haes et al. (20) described a p-[^18^F]MPPF binding study with microdialysis and PET scanning in conscious male rhesus monkeys. The specific activity of p-[^18^F]MPPF was >10 TBq/mmol (270 Ci/mmol) at the time of administration (TOA). The dose was given as a bolus–continuous infusion scheme to eliminate the possible effects of blood flow, with a mean injected activity of 420 ± 351 MBq (11.4 ± 9.5 mCi). The binding potentials (BPs) of p-[^18^F]MPPF in various monkey brain regions (n = 3) were estimated to be 0.4 ± 0.1, 0.5 ± 0.2, 1.1 ± 0.2, and 1.2 ± 0.4 for the striatum, raphe nucleus, frontal cortex, and hippocampus, respectively. Administration of fenfluramine, a serotonin-releasing agent and reuptake inhibitor, at i.v. doses of 5 or 10 mg/kg (90-130 min after p-[^18^F]MPPF injection) did not show significant changes in the BPs of p-[^18^F]MPPF. The authors suggested that the majority of 5-HT_1A_ receptors were in the low affinity state in the living monkey brain and that, therefore, the released 5-HT affected only a small percentage of the bound p-[^18^F]MPPF.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28p-%5B18F%5DMPPF%20OR%20%5B18F%5DMPPF%20OR%20F-18-MPPF%29%20AND%20human)]

Passchier et al. (21) studied the quantitative imaging of 5-HT_1A_ receptors with p-[^18^F]MPPF in 6 healthy volunteers. Each subject received 70 ± 18 MBq (1.9 ± 0.5 mCi) of p-[^18^F]MPPF with a specific activity of 95 ± 31 TBq/mmol (2565 ± 837 Ci/mmol) at TOA. The injected radioactivity was rapidly cleared from plasma and rapidly metabolized. Only 1% of p-[^18^F]MPPF remained in the plasma at 10 min. The authors found good correlation (r = 0.95) between the BPs and reported densities of 5-HT_1A_ receptors in various brain areas. A blocking experiment with pindolol (30 mg) showed a decrease of 40% in the region/cerebellum ratios of the target areas. In a similar study, the same group of researchers (22) found that the BPs of the medial temporal cortex, lateral temporal cortex, insular cortex, cingulate cortex, frontal cortex, striatum, and thalamus (n = 5) were 1.59 ± 0.31, 0.92 ± 0.07, 0.91 ± 0.16, 0.63 ± 0.11, 0.48 ± 0.09, 0.12 ± 0.13, and 0.10 ± 0.12, respectively. The lowest amounts of radioactivity were found in the cerebellum and basal ganglia.

In a study with 5 healthy volunteers, Costes et al. (23) quantified the parameters of ligand-receptor exchanges by use of a double-injection protocol (two p-[^18^F]MPPF bolus injections of 185 ± 9 MBq (5 ± 0.2 mCi) at a mean interval of 88.5 ± 4.2 min). A three-compartment ligand-receptor model was used to determine the kinetic parameters of 2 p-[^18^F]MPPF. The authors found a B_max_ of 2.9 pmol/ml and a K_d_ of 2.8 nmol/l in hippocampal regions. They also suggested that in the absence of blood arterial sampling, the BPs estimated by the Logan method would be a good index of local receptor concentrations in healthy subjects.

Sanabria-Bohorquez et al. (24) performed 60-min dynamic PET scans in 13 healthy volunteers after a single bolus injection of 3.7 MBq/kg (0.1 mCi/kg) p-[^18^F]MPPF (specific activity = 37-148 MBq/pmol (1-4 mCi/pmol) at the TOA). Metabolite quantification revealed that ~25% of total plasma activity was p-[^18^F]MPPF at 5 min. A plasma input function (PIF) method and a reference tissue method (RTM) were used to describe the kinetics parameters. The PIF method gave calculated BPs for the right and left hippocampus of 1.594 ± 0.274 and 1.576 ± 0.250, respectively, whereas the RTM gave corresponding BPs of 1.323 ± 0.193 and 1.301 ± 0.190, respectively.

Udo De Haes et al. (25) studied the effect of tryptophan depletion and infusion on p-[^18^F]MPPF binding in 6 healthy subjects. Each subject received 110-160 MBq (3-4.3 mCi) of p-[^18^F]MPPF (specific activity >10 TB/mmol (270 Ci/mmol) at the TOA), and [^15^O]H_2_O was used to assess regional cerebral blood flow. BPs were calculated with the simplified RTM. The mean changes in BPs for comparison of tryptophan depletion with tryptophan infusion were -0.6% in the medial temporal cortex, +1.9% in the cortical regions, and -16.6% in the raphe nucleus. The authors suggested that the induced changes in serotonin levels did not produce a significant effect on p-[^18^F]MPPF binding in human brains. Merlet et al. (26) found that the binding of p-[^18^F]MPPF to 5-HT_1A_ receptors in patients with refractory temporal lobe epilepsy (n = 9) was decreased in the epileptogenic temporal lobe. A decrease in BP was strongly correlated to the degree of epileptic activity. Praschak-Rieder et al. (27) reported that tryptophan depletion did not appear to have a significant effect on the regional brain BP of p-[^18^F]MPPF in 8 patients with major depressive disorder.

In a study designed to compile a normative database that included 27 female and 26 male healthy volunteers, Costes et al. (28) studied the possible influence of age and sex on p-[^18^F]MPPF BP, using a single injection of 192.7 ± 23.8 MBq (5.2 ± 0.6 mCi) of p-[^18^F]MPPF. They found a negative linear correlation between age and global p-[^18^F]MPPF BP values in females (a decrease of 3.6% per decade) but not in males. Male subjects in their 30s showed decreased binding in most cerebral regions compared with subjects in their 20s.

## NIH Support

NIH 1-PO1-MH48125-05, NS-24538, NIH NS-24538, MH-48125,

## References

1 Passchier J., van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
2 Bantick R.A., Rabiner E.A., Hirani E., de Vries M.H., Hume S.P., Grasby P.M. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
3. Sunderland, P.M., Structure and function of the nervous system, in Pathophysiology: The biologic basis for disease in adults and children, K.L. McCance, and S.H. Huether, Editor. 1994, Mosby-Year Book, Inc.: St. Louis, MO. p. 397-436.
4 Zhuang Z.P., Kung M.P., Chumpradit S., Mu M., Kung H.F. (1994). Derivatives of 4-(2'-methoxyphenyl)-1-[2'-(N-2"-pyridinyl-p-iodobenzamido)ethyl]pipera zine (p-MPPI) as 5-HT1A ligands. J Med Chem.
5 Zhuang Z.P., Kung M.P., Kung H.F. (1994). Synthesis and evaluation of 4-(2'-methoxyphenyl)-1-[2'-[N-(2"-pyridinyl)-p- iodobenzamido]ethyl]piperazine (p-MPPI): a new iodinated 5-HT1A ligand. J Med Chem.
6 Shiue C.Y., Shiue G.G., Mozley P.D., Kung M.P., Zhuang Z.P., Kim H.J., Kung H.F. (1997). P-[18F]-MPPF: a potential radioligand for PET studies of 5-HT1A receptors in humans. Synapse.
7 Le Bars D., Lemaire C., Ginovart N., Plenevaux A., Aerts J., Brihaye C., Hassoun W., Leviel V., Mekhsian P., Weissmann D., Pujol J.F., Luxen A., Comar D. (1998). High-yield radiosynthesis and preliminary in vivo evaluation of p-[18F]MPPF, a fluoro analog of WAY-100635. Nucl Med Biol.
8 Kung H.F., Stevenson D.A., Zhuang Z.P., Kung M.P., Frederick D., Hurt S.D. (1996). New 5-HT1A receptor antagonist: [3H]p-MPPF. Synapse.
9 Ma Y., Lang L., Kiesewetter D.O., Eckelman W.C. (2002). Liquid chromatography-tandem mass spectrometry identification of metabolites of three phenylcarboxyl derivatives of the 5-HT(1A) antagonist, N-(2-(4-(2-methoxyphenyl)-1-piperazinyl)ethyl)-N-(2-pyridyl) trans-4-fluorocyclohexanecarboxamide (FCWAY), produced by human and rat hepatocytes. J Chromatogr B Analyt Technol Biomed Life Sci.
10 Lang L., Jagoda E., Schmall B., Sassaman M., Ma Y., Eckelman W.C. (2000). Fluoro analogs of WAY-100635 with varying pharmacokinetics properties. Nucl Med Biol.
11 Thielen R.J., Fangon N.B., Frazer A. (1996). 4-(2'-Methoxyphenyl)-1-[2'-[N-(2"-pyridinyl)-p-iodobenzamido]ethyl] piperazine and 4-(2'-methoxyphenyl)-1-[2'-[N-(2"-pyridinyl)-p- fluorobenzamido]ethyl]piperazine, two new antagonists at pre- and postsynaptic serotonin-1A receptors. J Pharmacol Exp Ther.
12 Lang L., Jagoda E., Schmall B., Vuong B.K., Adams H.R., Nelson D.L., Carson R.E., Eckelman W.C. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
13 Plenevaux A., Weissmann D., Aerts J., Lemaire C., Brihaye C., Degueldre C., Le Bars D., Comar D., Pujol J., Luxen A. (2000). Tissue distribution, autoradiography, and metabolism of 4-(2'-methoxyphenyl)-1-[2' -[N-2"-pyridinyl)-p-[(18)F]fluorobenzamido]ethyl]piperazine (p-[(18)F]MPPF), a new serotonin 5-HT(1A) antagonist for positron emission tomography: An In vivo study in rats. J Neurochem.
14 Passchier J., van Waarde A., Doze P., Elsinga P.H., Vaalburg W. (2000). Influence of P-glycoprotein on brain uptake of [18F]MPPF in rats. Eur J Pharmacol.
15 Zimmer L., Mauger G., Le Bars D., Bonmarchand G., Luxen A., Pujol J.F. (2002). Effect of endogenous serotonin on the binding of the 5-hT1A PET ligand 18F-MPPF in the rat hippocampus: kinetic beta measurements combined with microdialysis. J Neurochem.
16 Zimmer L., Pain F., Mauger G., Plenevaux A., Le Bars D., Mastrippolito R., Pujol J.F., Renaud B., Laniece P. (2002). The potential of the beta-Microprobe, an intracerebral radiosensitive probe, to monitor the [(18)F]MPPF binding in the rat dorsal raphe nucleus. Eur J Nucl Med Mol Imaging.
17 Zimmer L., Rbah L., Giacomelli F., Le Bars D., Renaud B. (2003). A reduced extracellular serotonin level increases the 5-HT1A PET ligand 18F-MPPF binding in the rat hippocampus. J Nucl Med.
18 Rbah L., Leviel V., Zimmer L. (2003). Displacement of the PET ligand 18F-MPPF by the electrically evoked serotonin release in the rat hippocampus. Synapse.
19 Carson R.E., Wu Y., Lang L., Ma Y., Der M.G., Herscovitch P., Eckelman W.C. (2003). Brain uptake of the acid metabolites of F-18-labeled WAY 100635 analogs. J Cereb Blood Flow Metab.
20 Udo de Haes J.I., Cremers T.I., Bosker F.J., Postema F., Tiemersma-Wegman T.D., den Boer J.A. (2005). Effect of increased serotonin levels on [18F]MPPF binding in rat brain: fenfluramine vs the combination of citalopram and ketanserin. Neuropsychopharmacology.
21 Passchier J., van Waarde A., Pieterman R.M., Elsinga P.H., Pruim J., Hendrikse H.N., Willemsen A.T., Vaalburg W. (2000). Quantitative imaging of 5-HT(1A) receptor binding in healthy volunteers with [(18)f]p-MPPF. Nucl Med Biol.
22 Passchier J., van Waarde A., Pieterman R.M., Elsinga P.H., Pruim J., Hendrikse H.N., Willemsen A.T., Vaalburg W. (2000). In vivo delineation of 5-HT1A receptors in human brain with [18F]MPPF. J Nucl Med.
23 Costes N., Merlet I., Zimmer L., Lavenne F., Cinotti L., Delforge J., Luxen A., Pujol J.F., Le Bars D. (2002). Modeling [18 F]MPPF positron emission tomography kinetics for the determination of 5-hydroxytryptamine(1A) receptor concentration with multiinjection. J Cereb Blood Flow Metab.
24 Sanabria-Bohorquez S.M., Biver F., Damhaut P., Wikler D., Veraart C., Goldman S. (2002). Quantification of 5-HT(1A) receptors in human brain using p-MPPF kinetic modelling and PET. Eur J Nucl Med Mol Imaging.
25 Udo de Haes J.I., Bosker F.J., Van Waarde A., Pruim J., Willemsen A.T., Vaalburg W., Den Boer J.A. (2002). 5-HT(1A) receptor imaging in the human brain: effect of tryptophan depletion and infusion on [(18)F]MPPF binding. Synapse.
26 Merlet I., Ostrowsky K., Costes N., Ryvlin P., Isnard J., Faillenot I., Lavenne F., Dufournel D., Le Bars D., Mauguiere F. (2004). 5-HT1A receptor binding and intracerebral activity in temporal lobe epilepsy: an [18F]MPPF-PET study. Brain.
27 Praschak-Rieder N., Hussey D., Wilson A.A., Carella A., Lee M., Dunn E., Willeit M., Bagby R.M., Houle S., Meyer J.H. (2004). Tryptophan depletion and serotonin loss in selective serotonin reuptake inhibitor-treated depression: an [(18)F] MPPF positron emission tomography study. Biol Psychiatry.
28 Costes N., Merlet I., Ostrowsky K., Faillenot I., Lavenne F., Zimmer L., Ryvlin P., Le Bars D. (2005). A 18F-MPPF PET Normative Database of 5-HT1A Receptor Binding in Men and Women Over Aging. J Nucl Med.